# [^99m^Tc]Epidermal growth factor receptor–specific nanobody

Chemical name: | [^99m^Tc]Epidermal growth factor receptor–specific nanobody
Abbreviated name: | [^99m^Tc]EGFR nanobody
Synonym:
Agent Category: | Nanobody
Target: | Epidermal growth factor receptor
Target Category: | Antibody-receptor binding
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar imaging
Source of Signal/Contrast: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Click here for the human EGFR protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=11494380) and mRNA (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=41327737) sequence.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=EGFR+nanobody)]

A neoplastic tumor is the result of an altered expression of the proteins that regulate the survival and proliferation of a cell. The molecular changes associated with the development of tumors such as changed expression (up- or downregulation) of certain receptors or metabolic regulatory components in the cell are often used for the identification, diagnosis, and treatment of cancers or other pathological conditions. The molecular changes are usually detected with monoclonal antibodies (mAbs) developed against specific targets, and early detection of the cancer may result in the development of a suitable treatment and favorable outcome for the patient. To this end, mAbs may be labeled with radionuclides for noninvasive in vivo detection of the target tissue to diagnose a specific condition; techniques such as positron emission tomography and single-photon emission computed tomography (SPECT) are known to be sensitive enough to follow tumor binding and to image tumors with these radiolabeled mAbs (1, 2). However, the use of labeled mAbs has limitations because these molecules are relatively large and do not penetrate solid tumors; in addition they stay in blood circulation for a long time and tend to accumulate in the liver (3, 4). Investigators are constantly searching and evaluating alternatives to the conventional mAbs that have similar applications, but have superior production and stability characteristics.

One alternative to the conventional antibodies is the antibody variable fragment (Fv), genetically engineered by linking the variable-heavy (V_H_) and -light (V_L_) chain components of an antibody, which are also involved in antigen binding, through a flexible peptide linker to obtain a single-chain Fv (scFv) (5). The scFv has its limitations in that the peptide linkers are susceptible to enzymatic digestion under in vivo conditions, may show a reduced affinity toward the target, and tend to aggregate easily (6). Another alternative to the use of conventional antibodies is the use of a unique class of immunoglobulins found in the Camelidae species (camels and llamas) that consists of only the heavy chain component of the traditional mAb. These immunoglobulins contain a single variable domain that interacts with the antigen (7). These are the smallest, functional, antigen-binding fragments that can be produced from an immunoglobin, and the domains are known as VHH or a nanobody. Nanobodies are more stable than conventional mAbs and are inexpensively produced in a variety of expression systems such as yeast, filamentous fungi, or even plants (8-10). Also, nanobodies have reduced aggregation compared to the scFv fragments, and they have been shown to have low immunogenicity in mice because repeated administration in these animals did not evoke an anti-nanobody response (11).

The epidermal growth factor receptor (EGFR) has a characteristic overexpression in a variety of cancers such as those of the breast, ovaries, lungs, head and neck, bladder, and colon (12). EGFR is a 170-kDa transmembrane protein that promotes cell proliferation on binding of the autocrine epidermal growth factor (EGF) or the transforming growth factor α (TGFα), and EGFR operates through a receptor-associated tyrosine kinase–mediated signal transduction pathway. The progression of some cancers is attributed either to both organ increased level and activation of EGFR by EGF and TGFα or to a constitutive activation of the tyrosine kinase pathway caused by the development of a mutated receptor kinase. In an effort to develop therapy against cancers that are attributed to an increased EGFR activity or a mutated receptor kinase, a variety of EGFR inhibitors have been evaluated that either compete with EGF and TGFα for receptor binding (e.g., mAbs that target the receptor) or are small molecules that inhibit activation of the receptor tyrosine kinase signaling pathway (13). EGFR is the target of more than 350 clinical trials (http://clinicaltrials.gov/ct2/results?term=egfr) approved by the United States Food and Drug Administration. Roovers et al. (14) generated anti-EGFR nanobodies that were labeled with meta-stable technetium (^99m^Tc), and these nanobodies were used by Huang et al. to investigate molecular imaging (15) and by Gainkam et al. to study biodistribution and tumor imaging (16) in mice bearing xenograft tumors.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20synthesis)]

The EGFR nanobodies were generated as described by Roovers et al. (14). Briefly, Llama glama were immunized with human epidermal A431 carcinoma cells. Peripheral blood and lymph node lymphocytes from the immunized animals were then used to isolate a repertoire of the variable domains of the heavy-chain Abs, and subsequently a nanobody phage-display library was constructed for the variable domain heavy-chain Abs. The phage-display library was then panned to isolate a suitable clone using phage-enzyme-linked immunosorbent assays (ELISA). The genes coding for the EGFR-binding nanobody was recloned into an expression vector containing the c-Myc- and hexahistidine-tag coding sequences and expressed in Escherichia coli. The selected nanobodies were screened by ligand competition ELISA assays and were determined to have nanomolar affinities for the ligand (14).

The EGFR nanobody was labeled with ^99m^Tc through the C-terminal histidine tag with a ^99m^Tc-tricarbonyl intermediate [^99m^Tc(H_2_O)_3_(CO)_3_] using a commercially available kit (15). More than 90% of the radionuclide was incorporated by the nanobody, as determined with instant thin-layer chromatography (ITLC). The Rf values for the various labeled products separated during ITLC were not reported (15), so the labeled nanobody was used for the studies without further purification. The specific activity, stability, and radiochemical yield of the labeling reaction were not provided (15).

In another study, two different clones of the EGFR nanobody, 7C12 and 7D12, were labeled with ^99m^Tc with the commercial kit mentioned above and used for the biodistribution studies in mice bearing xenograft tumors (16). For the labeling, freshly prepared ^99m^Tc-pertechnetate was added to 6.6 nmol of the respective nanobodies in carbonate buffer (pH 8.0), and the mixture was incubated at 60°C for 90 min. The labeling efficiency values for 7C12 and 7D12 were reported to be 92.7 ± 1.3% and 95.4 ± 0.9%, respectively, as determined with ITLC. The labeled nanobodies were purified before use on a phosphate-buffered saline pre-equilibrated NAP-5 column only if the labeling yield was <90%. The specific activity of the labeled nanobodies was not reported (16).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=EGFR+nanobodies+in+vitro)]

The in vitro binding specificity of the nanobodies was determined with fluorescence-assisted cell-sorting analysis using Her14, DU145, A431, and NIH3T3 cells as negative controls (15). To determine whether the ^99m^Tc-labeled nanobodies could bind specifically to A431, which are EGFR-overexpressing cells, a competitive binding assay using an excess of unlabeled nanobodies was performed. The binding of the labeled nanobody was reported to be blocked by the unlabeled nanobody, indicating that the ^99m^Tc-labeled nanobody was specific for the receptor. Similar binding results were reported with ^99m^Tc-labeled 7C12 and the ^99m^Tc-labeled 7D12 nanobodies (16).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=anti-EGFR+nanobody+rodentia)]

The EGFR nanobodies were shown by Roovers et al. to be effective in delaying the outgrowth of A431-derived solid tumors in an in vivo murine xenograft model (14). Huang et al. investigated the ex vivo biodistribution of the [^99m^Tc]-EGFR nanobody in healthy mice (n = 6 animals) 3 h after administration of the radiolabel (15). The radioactivity was reported to accumulate mainly in the kidneys and the liver; minimal accumulation was observed in other organs. The nanobody had a half-life of 1.5 h for blood circulation and was cleared primarily through the kidneys. In the kidney accumulation of the radioactivity was 46.6 ± 0.9% total activity (% IA) compared with the liver uptake of 18.9 ± 0.6% IA. Pinhole SPECT imageing of mice bearing A431 or DU145 xenografts was performed 3 h after administration of the labeled nanobody. A higher uptake of the label was reported in the A431 tumors (5.2 ± 0.5% IA) compared with the DU145 xenografts (1.8 ± 0.3% IA; P < 0.001), which indicated that the labeled nanobody could discriminate between the tumors with high and moderate expression of EGFR (15).

In another study, the in vivo tumor uptake and biodistribution of two anti-EGFR nanobodies (7C12 and 7D12) labeled with ^99m^Tc were investigated (16). The ^99m^Tc-labeled 7C12 and ^99m^Tc-labeled 7D12 nanobodies were respectively administerd to mice (n=7 animals per nanobody group) bearing A431 (EGFR-positive) and R1M (EGFR-negative) cell xenograft tumors on separate days. The biodistribution and tumor targeting of the labeled compounds were assessed with SPECT imaging 1 h after administration of the label. Both nanobodies showed a similar high uptake (% IA) in the in A431 xenografts (4.55 ± 0.24 and 4.62 ± 0.36, respectively), and the uptake was low in the R1M tumors (1.16 ± 0.14 and 1.49 ± 0.60, respectively). Compared with ^99m^Tc-labeled 7D12, the uptake (% IA) of ^99m^Tc-labeled 7C12 after an intravenous administration was higher in the kidneys (63.48 ± 2.36 versus 56.25 ± 2.46) and lower in the liver (2.55 ± 0.26 versus 4.88 ± 0.86). Although both labeled nanobodies showed a similar short blood circulation half-life (<10 min), ^99m^Tc-labeled 7C12 showed a higher tumor accumulation (9.11 ± 1.12% IA) compared with ^99m^Tc-labeled 7D12 (6.09 ± 0.77% IA). Also, ^99m^Tc-labeled 7D12 had a higher blood activity compared to ^99m^Tc-labeled 7C12.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=EGFR+nanobody+non+human+primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=EGFR+nanobody+human+studies)]

No references are currently available.

## Supplemental Information

[Disclaimers]

## References

1 Larson S.M., Schoder H. (2008). Advances in positron emission tomography applications for urologic cancers. Curr Opin Urol.
2 Sharkey R.M., Karacay H., Vallabhajosula S., McBride W.J., Rossi E.A., Chang C.H., Goldsmith S.J., Goldenberg D.M. (2008). Metastatic human colonic carcinoma: molecular imaging with pretargeted SPECT and PET in a mouse model. Radiology.
3 Goldenberg D.M., Sharkey R.M. (2007). Novel radiolabeled antibody conjugates. Oncogene.
4 Burvenich I., Schoonooghe S., Cornelissen B., Blanckaert P., Coene E., Cuvelier C., Mertens N., Slegers G. (2005). In vitro and in vivo targeting properties of iodine-123- or iodine-131-labeled monoclonal antibody 14C5 in a non-small cell lung cancer and colon carcinoma model. Clin Cancer Res.
5 Jain M., Kamal N., Batra S.K. (2007). Engineering antibodies for clinical applications. Trends Biotechnol.
6 Whitlow M., Bell B.A., Feng S.L., Filpula D., Hardman K.D., Hubert S.L., Rollence M.L., Wood J.F., Schott M.E., Milenic D.E., et al. (1993). An improved linker for single-chain Fv with reduced aggregation and enhanced proteolytic stability. Protein Eng.
7 Revets H., De Baetselier P., Muyldermans S. (2005). Nanobodies as novel agents for cancer therapy. Expert Opin Biol Ther.
8 Frenken L.G., van der Linden R.H., Hermans P.W., Bos J.W., Ruuls R.C., de Geus B., Verrips C.T. (2000). Isolation of antigen specific llama VHH antibody fragments and their high level secretion by Saccharomyces cerevisiae. J Biotechnol.
9 Joosten V., Gouka R.J., van den Hondel C.A., Verrips C.T., Lokman B.C. (2005). Expression and production of llama variable heavy-chain antibody fragments (V(HH)s) by Aspergillus awamori. Appl Microbiol Biotechnol.
10 Ismaili A., Jalali-Javaran M., Rasaee M.J., Rahbarizadeh F., Forouzandeh-Moghadam M., Memari H.R. (2007). Production and characterization of anti-(mucin MUC1) single-domain antibody in tobacco (Nicotiana tabacum cultivar Xanthi). Biotechnol Appl Biochem.
11 Cortez-Retamozo V., Lauwereys M., Hassanzadeh Gh G., Gobert M., Conrath K., Muyldermans S., De Baetselier P., Revets H. (2002). Efficient tumor targeting by single-domain antibody fragments of camels. Int J Cancer.
12 Gullick W.J. (1991). Prevalence of aberrant expression of the epidermal growth factor receptor in human cancers. Br Med Bull.
13 Dancey J.E. (2003). Recent advances of molecular targeted agents: opportunities for imaging. Cancer Biol Ther.
14 Roovers R.C., Laeremans T., Huang L., De Taeye S., Verkleij A.J., Revets H., de Haard H.J. (2007). , and P.M. van Bergen en Henegouwen, Efficient inhibition of EGFR signaling and of tumour growth by antagonistic anti-EFGR Nanobodies.
15 Huang L., Gainkam L.O., Caveliers V., Vanhove C., Keyaerts M., De Baetselier P., Bossuyt A., Revets H., Lahoutte T. (2008). SPECT Imaging with (99m)Tc-Labeled EGFR-Specific Nanobody for In Vivo Monitoring of EGFR Expression. Mol Imaging Biol.
16 Gainkam L.O., Huang L., Caveliers V., Keyaerts M., Hernot S., Vaneycken I., Vanhove C., Revets H., De Baetselier P., Lahoutte T. (2008). Comparison of the Biodistribution and Tumor Targeting of Two 99mTc-Labeled Anti-EGFR Nanobodies in Mice, Using Pinhole SPECT/Micro-CT. J Nucl Med.